# ^76^Br-Human recombinant anti-ED-B fibronectin L19-small immunoprotein

Chemical name: | ^76^Br-Human recombinant anti-ED-B fibronectin L19-small immunoprotein
Abbreviated name: | ^76^Br-L19-SIP
Synonym: | ^76^Br-ED-B fibronectin-binding human antibody derivative
Agent Category: | Small immunoprotein (SIP)
Target: | ED-B Fibronectin (ED-B FN)
Target Category: | Antibody-antigen binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^76^Br
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=5725426), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=31406) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=407105) for more information about ED-B fibronectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(L19-SIP)+OR+(Labeled+human+recombinant+antibody+fragment+of+fibronectin))]

The ^76^Br-human recombinant anti-ED-B fibronectin L19-small immunoprotein (^76^Br-L19-SIP) is a radiolabeled molecular imaging agent developed for positron emission tomography (PET) imaging of tumor angiogenesis and guidance for antiangiogenic treatment (1). ^76^Br is a positron emitter with a 54% abundance and a half-life (t_½_) of 16.2 h.

Angiogenesis is a process of development and growth of new blood vessels from pre-existing vessels (2). Tumor growth depends on the formation of new blood vessels from this process. Normal angiogenesis is orderly and highly regulated, whereas tumor angiogenesis is chaotic and irregular. Abnormal angiogenesis is important in the carcinogenesis, growth, and progression of solid and hematologic tumors in humans (3). Fibronectins (FNs) are a family of universal cell-adhesion molecules that are widely distributed (4). FN is a polymorphic glycoprotein of ~2,500 amino acids and has a high molecular mass of 250–280 kDa. FN occurs in soluble form in plasma and other body fluids and in insoluble form in the extracellular matrices (5, 6). Both forms are dimers composed of a series of repeating units of three types and joined by two disulfide bonds at the C-terminus of the molecule. FN polymorphism arises from alternative splicing patterns of the pre-mRNA or post-translational modifications of FN itself (6). The splice variant ED-B FN is highly expressed during angiogenesis in both neoplastic and normal tissues (7), but higher levels of ED-B expression have been found in primary and metastatic tumors in breast, colorectal, and non-small cell lung cancers (4, 8-10).

Molecular imaging of angiogenesis offers serial non-invasive evaluation of both location and growth dynamics of tumors (11). PET or single-photon emission computed tomography imaging with an appropriate radiolabeled tracer targeted to angiogenic pathways may allow the evaluation of specific aspects of tumor vascular biology (10). A molecular probe that targets ED-B FN can be both an early tumor marker and a tool to monitor the success of antiangiogenic cancer therapy. The human recombinant single-chain antibody fragment (scFv) L19, which has a high affinity for ED-B FN, was developed by Pini et al. (12). Borsi et al (13). used the variable regions of L19 to construct a bivalent human SIP by fusing two scFvs to the _Є_CH_4_ domain of the secretory isoform S2 of human IgE (Є_s2_−CH_4_). The Є_s2_−CH_4_ domain provides a covalent stabilization of the dimer (molecular mass = ~80 kDa) (14). This group of researchers and Tijink et al (15) prepared radioiodinated L19-SIP that showed specific accumulation around tumor neovasculature and tumor stroma with high ED-B expression. In an effort to develop a PET molecular probe, Rossin et al. (1) used enzymatic radiobromination to prepare ^76^Br-L19-SIP and performed biodistribution and PET imaging studies in mice bearing the mouse embryonal teratocarcinoma F9. ^76^Br has relatively favorable production and photon yieldsand ^76^Br has a sufficiently long physical t_½_ for PET imaging up to 48 h after injection.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((L19-SIP)+OR+(Labeled+human+recombinant+antibody+fragment+of+fibronectin))+AND+synthesis)]

Pini et al. (12) constructed and used a large synthetic phage-display human antibody library (>3 × 10^8^ clones) to produce L19 with a very high affinity (dissociation constant (K_d_) = 54 pM) for the ED-B domain of FN. L19 was cloned in scFv configuration in the novel phagemid vector pDN332. Borsi et al. (13) reported the construction of the L19-SIP gene by DNA sequence amplification and insertion into the pUT-_Є_SIP vector. The L19-scFv was connected to the Є_s2_−CH_4_ domain by a short GGSG linker. The SIP gene was cloned into the mammalian expression vector pcDNA3 to obtain the construct pcDNA3-L19-SIP. This construct was used to transfect SP2/0 murine myeloma cells for expression. Immunoaffinity chromatography was used to purify the collected L19-SIP. Rossin et al. (1) prepared ^76^Br-L19-SIP based on a modified enzymatic method of Lovqvist et al. (16). Briefly, ^76^Br-labeled bromide was produced by the ^76^Se(p,n)^76^Br nuclear reaction on a ^76^Se-enriched Cu_2_Se target and recovered by dry distillation. L19-SIP was mixed with ^76^Br-labeled bromide and 0.6 U bromoperoxidase in 300 μl 50 mmol/L phosphate buffer (pH 7.0) containing 80 μmol/L hydrogen peroxide. The reaction mixture was incubated at 0ºC for 80 min. When <37 MBq (1 mCi) ^76^Br was used, the radiolabeling yield was 82 ± 2% (n = 4). For >37 MBq (1 mCi) ^76^Br, the radiochemical yield was 55% (n = 2). Analysis with radio-fast-protein liquid chromatography (radio-FPLC) showed that the ^76^Br-L19-SIP used for animal experiments had a radiochemical purity >90%. The specific activity was not reported, but the dose for the animal biodistribution studies was ~185 kBq/μg (5 μCi/μg) or ~14.8 kBq/pmol (0.4 μCi/pmol) based on the molecular mass of ~80 kDa, and the dose for the imaging study was ~440 kBq/μg (11.89 μCi/μg) or 35.2 kBq/pmol (0.95 μCi/pmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((L19-SIP)+OR+(Labeled+human+recombinant+antibody+fragment+of+fibronectin))+AND+in+vitro)]

Rossin et al. (1) determined the in vitro immunoreactivity of ^76^Br-L19-SIP to be 80 ± 2% (n = 5) by affinity chromatography. The in vitro stability of ^76^Br-L19-SIP was studied by incubating the radioligand in mouse serum at 37ºC. After 48 h incubation, radio-FPLC analysis detected no free ^76^Br-labeled bromide, but 21% of the yield comprised of high molecular weight impurities.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((L19-SIP)+OR+(Labeled+human+recombinant+antibody+fragment+of+fibronectin))AND+mice)]

Biodistribution studies (n = 3–4) of ^76^Br-L19-SIP were performed in mice bearing subcutaneous mouse embryonal teratocarcinoma F9 tumors (0.1–2.8 g) (1). F9 tumors were previously reported to express high levels of ED-B FN (13). Each mouse received ~1.3 MBq (35 μCi) ^76^Br-L19-SIP (~185 kBq/μg or 5 μCi/μg) or ~0.35 mg antibody/kg body weight by i.v. administration. ^76^Br-L19-SIP showed high radioactivity localization in the tumor but slow clearance from the blood and blood-rich organs. The tumor radioactivity levels of ^76^Br-L19-SIP, expressed as percentage of injected dose per gram (% ID/g), were 18.1 ± 7.6 (5 h), 9.3 ± 3.5 (24 h), and 14.3 ± 1.6 (48 h). The tumor/blood ratios were 0.8 ± 0.4 (5 h), 1.2 ± 0.5 (24 h), and 1.8 ± 0.4 (48 h). The tumor/muscle ratios were 7.3 ± 3.1 (5 h), 2.3 ± 1.1 (24 h), and 5.6 ± 0.6 (48 h). There were also high radioactivity levels in the mouse reproductive organs (uterus and ovaries), which express the ED-B fibronectin. At 5 h, the radioactivity levels (% ID/g) in other major organs were 7.0 ± 2.3 (ovaries), 22.4 ± 3.7 (blood), 11.4 ± 2.0 (lung), 5.0 ± 0.3 (liver), 5.7 ± 0.6 (spleen), 5.5 ± 2.5 (thyroid), 13.5 ± 6.3 (uterus), 9.4 ± 1.9 (kidney), 6.2 ± 0.6 (heart), 2.5 ± 0.2 (muscle), and 3.6 ± 0.6 (bone). By 48 h, these radioactivity levels (% ID/g) decreased to 1.8 ± 0.3 (ovaries), 8.1 ± 1.7 (blood), 5.8 ± 0.9 (lung), 2.5 ± 0.5 (liver), 2.9 ± 0.7 (spleen), 2.4 ± 0.3 (thyroid), 6.0 ± 1.0 (uterus), 4.1 ± 1.2 (kidney), 2.7 ± 0.5 (heart), 2.6 ± 0.0 (muscle), and 2.6 ± 0.4 (bone). Renal elimination was slow with only 4.7 ± 0.9% ID at 48 h. No specific blocking study was performed.

Metabolic studies of ^76^Br-L19-SIP were conducted in normal mice (n = 3) (1). Each mouse received ~1.8 MBq (48.65 μCi) ^76^Br-L19-SIP (~0.2 mg/kg body weight) by i.v. administration. In the serum, radio-FPLC analysis showed that the amounts of intact ^76^Br-L19-SIP were 86.1 ± 1.7%, 73.5 ± 0.5%, and 24.7 ± 0.9% at 2 h, 5 h, and 24 h after injection, respectively. The immunoreactivity of these samples were 65%, 66%, and 21%, respectively. In the urine, the majority of the radioactivity was ^76^Br-labeled bromide. The amounts of intact ^76^Br-L19-SIP were 7.7 ± 0.1%, 5.8 ± 0.6%, and 0.8 ± 0.3% at 2 h, 5 h, and 24 h, respectively, in urine.

PET imaging was performed in mice (n = 4) bearing subcutaneous F9 tumors (0.1–2.8 g) (4). Each mouse was injected with ~13 MBq (351 μCi) ^76^Br-L19-SIP (~440 kBq/μg or 11.89 μCi/μg) by i.v. administration. Microcomputed tomography imaging studies were also performed for landmark registration. Imaging with ^76^Br-L19-SIP produced clear tumor images at 5, 24, and 48 h. The radioactivity distribution pattern was similar to the biodistribution studies. The background radioactivity in the abdominal area was high. The kidneys, heart, and aorta were visualized at earlier time points. The stomach and bladder were visualized at 48 h. The tumor standard uptake values (radioactivity concentration in μCi/ml divided by the injected dose in μCi/animal weight in g) obtained by semiquantitative analysis of microPET images were 2.4 ± 0.5 (5 h), 2.7 ± 0.1 (24 h), and 2.4 ± 0.2 (48 h).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((L19-SIP)+OR+(Labeled+human+recombinant+antibody+fragment+of+fibronectin))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((L19-SIP)+OR+(Labeled+human+recombinant+antibody+fragment+of+fibronectin))++AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((L19-SIP)+OR+(Labeled+human+recombinant+antibody+fragment+of+fibronectin))AND+human)]

No publication is currently available.

## References

1 Rossin R., Berndorff D., Friebe M., Dinkelborg L.M., Welch M.J. (2007). Small-animal PET of tumor angiogenesis using a (76)Br-labeled human recombinant antibody fragment to the ED-B domain of fibronectin. J Nucl Med.
2 Shinkaruk S., Bayle M., Lain G., Deleris G. (2003). Vascular endothelial cell growth factor (VEGF), an emerging target for cancer chemotherapy. Curr Med Chem Anticancer Agents.
3 Ranieri G., Patruno R., Ruggieri E., Montemurro S., Valerio P., Ribatti D. (2006). Vascular endothelial growth factor (VEGF) as a target of bevacizumab in cancer: from the biology to the clinic. Curr Med Chem.
4 Berndorff D., Borkowski S., Moosmayer D., Viti F., Muller-Tiemann B., Sieger S., Friebe M., Hilger C.S., Zardi L., Neri D., Dinkelborg L.M. (2006). Imaging of tumor angiogenesis using 99mTc-labeled human recombinant anti-ED-B fibronectin antibody fragments. J Nucl Med.
5 Carnemolla B., Balza E., Siri A., Zardi L., Nicotra M.R., Bigotti A., Natali P.G. (1989). A tumor-associated fibronectin isoform generated by alternative splicing of messenger RNA precursors. J Cell Biol.
6 Kosmehl H., Berndt A., Katenkamp D. (1996). Molecular variants of fibronectin and laminin: structure, physiological occurrence and histopathological aspects. Virchows Arch.
7 Castellani P., Viale G., Dorcaratto A., Nicolo G., Kaczmarek J., Querze G., Zardi L. (1994). The fibronectin isoform containing the ED-B oncofetal domain: a marker of angiogenesis. Int J Cancer.
8 Kaczmarek J., Castellani P., Nicolo G., Spina B., Allemanni G., Zardi L. (1994). Distribution of oncofetal fibronectin isoforms in normal, hyperplastic and neoplastic human breast tissues. Int J Cancer.
9 Pujuguet P., Hammann A., Moutet M., Samuel J.L., Martin F., Martin M. (1996). Expression of fibronectin ED-A+ and ED-B+ isoforms by human and experimental colorectal cancer. Contribution of cancer cells and tumor-associated myofibroblasts. Am J Pathol.
10 Santimaria M., Moscatelli G., Viale G.L., Giovannoni L., Neri G., Viti F., Leprini A., Borsi L., Castellani P., Zardi L., Neri D., Riva P. (2003). Immunoscintigraphic detection of the ED-B domain of fibronectin, a marker of angiogenesis, in patients with cancer. Clin Cancer Res.
11. Laking, G.R. and P.M. Price, Positron emission tomographic imaging of angiogenesis and vascular function. Br J Radiol, 2003. 76 Spec No 1: p. S50-9.
12 Pini A., Viti F., Santucci A., Carnemolla B., Zardi L., Neri P., Neri D. (1998). Design and use of a phage display library. Human antibodies with subnanomolar affinity against a marker of angiogenesis eluted from a two-dimensional gel. J Biol Chem.
13 Borsi L., Balza E., Bestagno M., Castellani P., Carnemolla B., Biro A., Leprini A., Sepulveda J., Burrone O., Neri D., Zardi L. (2002). Selective targeting of tumoral vasculature: comparison of different formats of an antibody (L19) to the ED-B domain of fibronectin. Int J Cancer.
14 El-Emir E., Dearling J.L., Huhalov A., Robson M.P., Boxer G., Neri D., van Dongen G.A., Trachsel E., Begent R.H., Pedley R.B. (2007). Characterisation and radioimmunotherapy of L19-SIP, an anti-angiogenic antibody against the extra domain B of fibronectin, in colorectal tumour models. Br J Cancer.
15 Tijink B.M., Neri D., Leemans C.R., Budde M., Dinkelborg L.M., Stigter-van Walsum M., Zardi L., van Dongen G.A. (2006). Radioimmunotherapy of head and neck cancer xenografts using 131I-labeled antibody L19-SIP for selective targeting of tumor vasculature. J Nucl Med.
16 Lovqvist A., Sundin A., Ahlstrom H., Carlsson J., Lundqvist H. (1997). Pharmacokinetics and experimental PET imaging of a bromine-76-labeled monoclonal anti-CEA antibody. J Nucl Med.